# ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-polyethylene-glycol-single-walled nanotube-c(RGDyK)

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-polyethylene-glycol-single-walled nanotube-c(RGDyK)
Abbreviated name: | ^64^Cu-DOTA-SWNT-PEG-c(RGDyK)
Synonym:
Agent category: | Peptide
Target: | Integrin α_v_β_3_
Target category: | Receptor
Method of detection: | PET
Source of signal\contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4504763), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=40217844) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3685) for more information about integrin α_v_β_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+SWNT)]

Optical fluorescence imaging is increasingly used to visualize biological functions of specific targets (1, 2). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging in small animals.

Carbon nanotubes are made of carbon fullerene carbon units, which respond to local dielectric changes without photobleaching (3, 4). They can be tuned in a range of wavelengths for NIR absorption, thus providing broad excitation profiles and high absorption coefficients. They can be coated and capped with hydrophilic materials for additional conjugation with biomolecules, such as peptides, antibodies, nucleic acids, and small organic compounds for in vitro and in vivo studies (5). Single-walled carbon nanotubes (SWNTs) have a diameter of 1–5 nm and a length of 200–1,000 nm, and they have been shown to be non-toxic to cells in vitro (6). However, there have been limited in vivo studies of SWNT toxicological and pharmacological profiles in small animals.

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (7). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (8-13). Expression of the α_v_β_3_ integrin is strong in tumor cells and activated endothelial cells, whereas expression is weak in resting endothelial cells and most normal tissues. Antagonists of α_v_β_3_ are being studied as antitumor and antiangiogenic agents and the agonists of α_v_β_3_ are being studied as angiogenic agents for coronary angiogenesis (12, 14, 15). A peptide sequence consisting of Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various ligands have been introduced for imaging of tumors and tumor angiogenesis (16). Liu et al. (17) conjugated ^64^Cu-1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (^64^Cu-DOTA) and c(RGDyK) to phospholipid-polyethylene-glycol (PL-PEG)–coated SWNTs (^64^Cu-DOTA-SWNT-PEG-c(RGDyK)) for imaging α_v_β_3_ integrin expression in tumors and their vasculatures.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+SWNT+synthesis)]

Liu et al. (17) performed sonication of SWNTs in a solution of PL-PEG_4500_-NH_2_ for 1 h to obtain SWNT-PEG_4500_-NH_2_, which exhibits a molar extension coefficient of 7.9 × 10^6^ M^-1^cm^-1^ at 808 nm absorbance. The average length of the SWNTs was ~200 nm. SWNT-PEG_4500_-NH_2_ nanotubes were incubated with DOTA-N-hydroxysulfonosuccinimide (SNHS) for 4 h (pH 7.4) to form SWNT-PEG_4500_-DOTA; there were ~62 DOTA molecules per SWNT. To prepare conjugates with both DOTA and RGD, DOTA-SNHS and sulphosuccinimidyl 4-N-maleimidomethyl cyclohexane-1-carboxylate were mixed at 1:5 molar ratios and incubated in SWNT-PEG-NH_2_ solutions for 2 h (pH 7.4). The resulted SWNTs were reacted overnight with 0.2 mM thiolated c(RGDyK) in the presence of 10 mM Tris(2-carboxyethyl) phosphine hydrochloride (pH 7.4), yielding DOTA-SWNT-PEG_5400_-RGD with both RGD and DOTA on the SWNTs. There were 36.2 c(RGDyK) molecules per SWNT with a c(RGDyK)/DOTA ratio of 0.59. DOTA-SWNT-PEG_2000_-RGD was prepared similarly with the use of PL-PEG_2000_-NH_2_. There were 47.4 c(RGDyK) molecules per SWNT with a c(RGDyK)/DOTA ratio of 0.71. ^64^CuCl_2_ (74 MBq (2 mCi)) was added to 150 nM SWNT conjugates in 0.1 M NaOAc solution (pH 6.5). The reaction mixture was incubated for 1 h at 40°C. The radiolabeled yield was 60–80% with a specific activity of ~370 MBq/µmol (~10 mCi/µmol). ^64^Cu-SWNT conjugates in mouse serum remained intact at 37°C after 24 h incubation.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+SWNT+in+vitro)]

Liu et al. (17) performed in vitro inhibition studies of DOTA-SWNT-PEG_5400_-RGD and DOTA-SWNT-PEG_2000_-RGD in cultured U87MG human glioblastoma cells with ^125^I-echistatin. The 50% inhibition concentration values for DOTA-SWNT-PEG_5400_-RGD and DOTA-SWNT-PEG_2000_-RGD were 11.1 and 4.1 nM, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+SWNT+%20rodentia)]

Liu et al. (17) performed biodistribution studies of ^64^Cu-DOTA-SWNT-PEG_5400_-RGD and ^64^Cu-DOTA-SWNT-PEG_2000_-RGD in nude mice (n = 3 mice/group) bearing U87MG tumors after injection of 7.4–11.1 MBq (0.2–0.3 mCi) of the tracers. Tracer accumulation in the α_v_β_3_-integrin-expressing U87MG tumor was higher for ^64^Cu-DOTA-SWNT-PEG_5400_-RGD (~13% injected dose (ID)/g) than ^64^Cu-DOTA-SWNT-PEG_2000_-RGD (~4% ID/g) at 24 h. The highest radioactive concentration was found in the liver with ~19% ID/g for ^64^Cu-DOTA-SWNT-PEG_4500_-RGD and ~28% ID/g for ^64^Cu-DOTA-SWNT-PEG_2000_-RGD. On the other hand, the spleen, kidney, and lung accumulated ~5% ID/g for both tracers. ^64^Cu-DOTA-SWNT-PEG_5400_ and ^64^Cu-DOTA-SWNT-PEG_2000_ exhibited biodistribution similar to their RGD conjugates with only 3–4% ID/g radioactivity in the tumor. ^64^Cu-DOTA-SWNT-PEG_2000_ (~35% ID/g) also exhibited a higher liver accumulation than ^64^Cu-DOTA-SWNT-PEG_4500_ (~19% ID/g). ^64^Cu-DOTA-SWNT-PEG_5400_ (~2 h) exhibited a longer blood half-life than ^64^Cu-DOTA-SWNT-PEG_2000_ (~0.5 h). Positron emission tomography imaging in nude mice bearing U87MG tumors with the ^64^Cu-DOTA-SWNT conjugates visualized the tumors at 0.5, 6, 18, and 24 h. ^64^Cu-DOTA-SWNT-PEG_5400_ and ^64^Cu-DOTA-SWNT-PEG_2000_ exhibited only 3–4% ID/g in the tumor, whereas ^64^Cu-DOTA-SWNT-PEG_5400_-RGD and ^64^Cu-DOTA-SWNT-PEG_2000_-RGD exhibited ~15% ID/g and ~5% ID/g at 24 h, respectively. Tumor accumulation was rapid and reached a plateau at 6 h. Tumor/muscle ratio was >15 for ^64^Cu-DOTA-SWNT-PEG_5400_-RGD. There was relatively low radioactivity elsewhere (except the liver) in the mice, confirming the biodistribution data. ^64^Cu-DOTA-SWNT-PEG_2000_ exhibited a higher liver accumulation than ^64^Cu-DOTA-SWNT-PEG_4500_ as shown in the biodistribution studies. Co-administration of c(RGDyK) with ^64^Cu-DOTA-SWNT-PEG_5400_-RGD inhibited tumor accumulation by ~75%. Low tumor accumulation (~3% ID/g) of ^64^Cu-DOTA-SWNT-PEG_5400_-RGD was observed in mice bearing HT-29 tumors (α_v_β_3_-integrin negative). Raman spectroscopy analysis (SWNTs, G band, ~1,600 cm^-1^) of various tissues confirmed the co-localization of SWNTs and ^64^Cu.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+SWNT+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+SWNT+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+SWNT+human)]

No publication is currently available.

## NIH Support

R21 EB001785, R21 CA102123, P50 CA114747, R24 CA93862, U54 CA93862

## References

1 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
2 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
3 Hersam M.C. (2008). Progress towards monodisperse single-walled carbon nanotubes. Nat Nanotechnol.
4 Barone P.W., Baik S., Heller D.A., Strano M.S. (2005). Near-infrared optical sensors based on single-walled carbon nanotubes. Nat Mater.
5 Klumpp C., Kostarelos K., Prato M., Bianco A. (2006). Functionalized carbon nanotubes as emerging nanovectors for the delivery of therapeutics. Biochim Biophys Acta.
6 Chin S.F., Baughman R.H., Dalton A.B., Dieckmann G.R., Draper R.K., Mikoryak C., Musselman I.H., Poenitzsch V.Z., Xie H., Pantano P. (2007). Amphiphilic helical peptide enhances the uptake of single-walled carbon nanotubes by living cells. Exp Biol Med (Maywood).
7 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
8 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
9 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
10 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
11 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
12 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
13 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
14 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
15 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
16 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
17 Liu Z., Cai W., He L., Nakayama N., Chen K., Sun X., Chen X., Dai H. (2007). In vivo biodistribution and highly efficient tumour targeting of carbon nanotubes in mice. Nat Nanotechnol.